# 2-(2-Nitroimidazol-1H-yl)-(3-[^18^F]fluoropropyl)acetamide

Chemical name: | 2-(2-Nitroimidazol-1H-yl)-N-(3-[^18^F]fluoropropyl)acetamide
Abbreviated name: | [^18^F]EF1
Synonym: | [^18^F]-2-(2-Nitro-1H-imidazol-1-yl)-N-(3-fluoropropyl)acetamide
Agent Category: | Compound
Target: | Hypoxic cells
Target Category: | Intracellular reduction and binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5BAll%20Fields%5D%20AND%20EF1%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D)]

Hypoxia in malignant tumors is thought to be a major factor limiting the efficacy of chemotherapy and radiotherapy, and its accurate diagnosis is considered a very important and urgent problem to address. This has led to the search and development of hypoxia-targeted, non-invasive markers of tumor hypoxia. Among those markers, [^18^F]-labeled nitroimidazoles, used in conjunction with positron emission tomography (PET), offer an alternative that is less invasive and less prone to sampling error than the Eppendorf (oxygen) electrode method (1, 2).

Fluoromisonidazole ([^18^F]FMISO) is the most widely used nitroimidazole derivate used with PET. Novel 2-nitroimidazoles, such as [^18^F]FETA (3), [^18^F]FETNIM (4), 4-Br[^18^F]FPN (5), [^18^F]EF1, and [^18^F]EF5 (6), are currently being investigated as potential markers of tumor hypoxia.

[^18^F]EF1 is a molecule comparable to [^18^F]FETA, with the exception that [^18^F]EF1 carries an additional carbon on the side chain. [^18^F]EF1 is also a 3-monofluorinated analog of the pentafluorinated molecule EF5 (2-(2-nitro-1H-imidazol-1-yl)-N-(2,2,3,3,3-[^18^F]pentafluoropropyl)acetamide), which is used for the measurement of hypoxia in immunohistochemistry (7) and flow cytometry (8).

The oxygen-dependent metabolism of nitroimidazoles is an intracellular process consisting of a series of one-electron reductions. The nitro-radical anion produced in the first reduction step is very reactive toward oxygen, leaving no substrate for the second step of the reduction process. In contrast, a low-oxygen environment induces further reductive reactions that ultimately lead to the formation of either reactive products that can covalently bind to cell components or to charged species that diffuse slowly out of the tissues (1). The reactive products observed during this multi-step process include nitroso (2e-), hydroxylamine (4e-), and amine (6e-) derivatives. When the fragmentation of the imidazole ring occurs, reactive portions of the molecule, such as glyoxal, bind to macromolecular components of cells in tissues and tumors (2).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5BAll%20Fields%5D%20AND%20EF1%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D)]

Two modes of synthesis for [^18^F]EF1 were reported in 1999 by Kachur et al. (9).

In the first mode, EF1 is synthesized from EBr1 by a nucleophilic substitution of bromine by fluorine using potassium Kryptofix 222 fluoride in dimethyl sulfoxide (DMSO). EBr1 is prepared from 2-(2-nitroimidazol-1H-yl)-acetic acid and 3-bromopropylamine hydrobromide using the mixed anhydride reaction with isobutyl chloroformate (10). After dissolution in acetonitrile (MeCN) and storage over molecular sieves, the mixture is cooled to 0ºC under argon and stirred with an addition of isobutylchloroformate. A solution of 3-bromopropylamine hydrobromide (219 mg, 1 mmol) and 140 μl of NEt_3_ (1 mmol) in 5 ml of MeCN is then added. After stirring, cooling to 0°C, and centrifugation, the resulting precipitate of NEt_3_H^+^Cl− is extracted and dried at room temperature. The final product, EBr1, is then recrystallized from hexane/EtOAc (10:1 ratio) and dried over molecular sieves. EBr1 is obtained with a yield of approximately 70%.

In the second mode, EF1 is prepared by following the protocol used for EBr1 described above, except that an equivalent quantity of 3-fluoro- instead of 3-bromopropylamine is used. In this case, the C–F bond in EF1 (which is not hydrolyzed) reacts with an excess of triethylamine (unlike the C–Br bond in EBr1). In this second method, the reaction conditions and separation procedure are different: a 2-fold excess of triethylamine is used in the reaction, and the dried reaction mixture, after centrifugation, is dissolved in dry EtOAc. After evaporation and dissolution of the residue in CHCl_3_, EF1 is extracted by H_2_O, and the aqueous layers are then combined and lyophilized. The yield is approximately 15% pure EF1.

The preparation of the radioactive carrier is performed by using [^18^F]fluoride, obtained by the ^18^O(p,n) ^18^F reaction using ^18^O-enriched water. Details for this preparation are reported by Kachur et al. (9).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5BAll%20Fields%5D%20AND%20EF1%5BAll%20Fields%5D%20AND%20%28%22in%20vitro%22%5BMeSH%20Terms%5D%20OR%20in%20vitro%5BText%20Word%5D%29)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29EF1%20AND%20%22rodentia%22%5BMeSH%20Terms%5D)]

Evans et al. (11) showed the ability of [^18^F]EF1 to differentiate hypoxic versus aerobic tumors in rodents, using the hypoxic Morris 7777 (Q7) hepatoma tumor type and the oxic 9LF glioma tumor model. The experimental procedure involved injecting intravenously approximately 1.9 MBq (0.05 mCi) of [^18^F]EF1 (1% of the animal’s weight), 3 mM of the carrier EF1,and 7 mM EF3 (2-(2-nitro-1H-imidazol-1-yl)-N-(2,2,3,3,3-[^18^F]trifluoropropyl)acetamide). The specific activity of [^18^F]EF1 for injection was 5.6 × 10^4^ MBq/mol (1.51 × 10^3^ mCi/mol).

The use of an excess of the carrier drug EF1 and EF3 made it possible to make an independent assessment of the drug biodistribution by more conventional means (e.g., high-performance liquid chromatography (HPLC)), as well as making an immunohistochemical detection of intracellular EF1/EF3 adducts in the tumors using EF3-specific antibodies. Biodistribution of [^18^F]EF1 was also performed in non-tumor-bearing mice, as a reference. After positron emission tomography (PET) studies, the tissues for all animals were removed and analyzed by γ-counting at 1, 5, 90, and 120 min after injection.

Results showed that for both rat tumor types, low retention of [^18^F]EF1 was obtained in muscle, heart, spleen and brain, whereas significantly higher levels were found in tumor and bone (tibia). γ-counts of excised organs and tissues were measured at 90 min after injection, and their uptake was expressed as a percentage of injected activity per gram of sample (% ID/g). The following results (% ID/g) were found for muscle, heart, spleen, brain, tumor, and bone (tibia), respectively (all values are x 10−^3^): for Q7 tumors, 2.5, 1.5, 3.0, 1.5, 6.5, and 13; for 9LF tumors, 1.5, 1.0, 1.8, 0.6, 2.5, and 12 (11).

Studies using normal mice showed a rapid decrease of activity in all organs except bone (tibia), likely reflecting a bone contamination by [^18^F]F^-^ and a very substantial increase of urine activity by 90 min after injection (0.6 fraction ID/g). For Q7 tumors, the tumor-to-muscle ratio (T/M) initially decreased (from approximately 2.0 at 10 min after injection to 1.7 at 50 min) and then increased (to approximately 2.4) to reach a plateau 125 min after injection. In contrast, the T/M ratio for 9L tumors never exceeded 1.0, and a steady decrease was observed over time (11).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29EF1%20AND%20%28dog%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29EF1%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29EF1%20AND%20human)]

No publication is currently available.

## References

1 Nunn A, Linder K, Strauss HW. (1995). Nitroimidazoles and imaging hypoxia. Eur J Nucl Med.
2 Hodgkiss RJ. (1998). Use of 2-nitroimidazoles as bioreductive markers for tumour hypoxia. Anticancer Drug Des.
3 Rasey JS, Hofstrand PD, Chin LK, Tewson TJ. (1999). Characterization of [18F]fluoroetanidazole, a new radiopharmaceutical for detecting tumor hypoxia. J Nucl Med.
4 Yang DJ, Wallace S, Cherif A, Li C, Gretzer MB, Kim EE, Podoloff DA. (1995). Development of F-18-labeled fluoroerythronitroimidazole as a PET agent for imaging tumor hypoxia. Radiology.
5 Yamamoto F, Aoki M, Furusawa Y, Ando K, Kuwabara Y, Masuda K, Sasaki S, Maeda M. (2002). Synthesis and evaluation of 4-bromo-1-(3-[18F]fluoropropyl)-2-nitroimidazole with a low energy LUMO orbital designed as brain hypoxia-targeting imaging agent. Biol Pharm Bull.
6 Dolbier WR, Li AR, Koch CJ, Shiue CY, Kachur AV. (2001). [18F]-EF5, a marker for PET detection of hypoxia: synthesis of precursor and a new fluorination procedure. Appl Radiat Isot.
7 Evans SM, Joiner B, Jenkins WT, Laughlin KM, Lord EM, Koch CJ. (1995). Identification of hypoxia in cells and tissues of epigastric 9L rat glioma using EF5. Br J Cancer.
8 Evans SM, Jenkins WT, Joiner B, Lord EM, Koch CJ. (1996). 2-Nitroimidazole (EF5) binding predicts radiation resistance in individual 9L s.c. tumors. Cancer Res.
9 Kachur AV, Dolbier WR, Evans SM, Shiue CY, Shiue GG, Skov KA, Baird IR, James BR, Li AR, Roche A, Koch CJ. (1999). Synthesis of new hypoxia markers EF1 and [18F]-EF1. Appl Radiat Isot.
10 Krejcarek GE, Tucker KL. (1977). Covalent attachment of chelating groups to macromolecules. Biochem Biophys Res Commun.
11 Evans SM, Kachur AV, Shiue CY, Hustinx R, Jenkins WT, Shive GG, Karp JS, Alavi A, Lord EM, Dolbier WR, Koch CJ. (2000). Noninvasive detection of tumor hypoxia using the 2-nitroimidazole [18F]EF1. J Nucl Med.